# 5-(6-(5-[^11^C]methylhexahydropyrrolo[3,4-c]pyrrol-2(1H)-yl)pyridazin-3-yl)-1H-indole

Chemical name: | 5-(6-(5-[^11^C]methylhexahydropyrrolo[3,4-c]pyrrol-2(1H)-yl)pyridazin-3-yl)-1H-indole
Abbreviated name: | [^11^C]A-833834
Synonym:
Agent Category: | Compound
Target: | α7-Nicotinic acetylcholine receptor (α7-nAChR)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the structure of [^11^C]A-833834 for more information in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=A-833834&cmd=DetailsSearch)]

The nicotinic acetylcholine receptors (nAChR) are pentameric ligand-gated cation channels that are found primarily in the central nervous system of mammals and are composed of α and β subunits arranged in various homomeric or heteromeric stoichiometric arrangements (for details, see dos Santos Coura and Granon (1)). The nAChRs have a high affinity for both nicotine and acetylcholine; binding of a ligand to the receptor facilitates the passage of cations into the cell, which alters the polarity of the cell membrane and activates the signal transduction pathways that culminate in a cellular response (2). These receptors are believed to be involved in a variety of cognitive functions and memory (1), neuroprotection in Parkinson’s disease (3), Alzheimer’s disease (AD) (4), and the progression of certain cancers (5). The heteromeric α4β2 and the homomeric α7 are the most commonly expressed nAChRs in the brain, and the β2 subunit is a component of most heteromeric nicotinic receptors in the central nervous system. There is much evidence that α4β2-nAChR is involved in normal cognitive functions in animals; it is also implicated in addiction (e.g., smoking) and the cognitive impairments observed in AD, attention deficit hyperactivity disorder, and schizophrenia (6). α7-nAChR participates in cognition and has a reduced expression in the human schizophrenic brain, and there are indications that it has a therapeutic role in the treatment of AD (7).

Although some radiolabeled compounds can be used with positron emission tomography (PET) to visualize α4β2-nAChR in the human brain these radio-ligands exhibit slow kinetics and a low binding potential in the brain which limits their use to investigate nAChR in humans (8). Therefore, no suitable tracer(s) are available for the noninvasive imaging of α7-nAChR in humans (7). In an effort to develop new ligands for α7-nAChR two compounds, 5-(6-(5-methylhexahydropyrrolo[3,4-c]pyrrol-2(1H)-yl)pyridazin-3-yl)-1H-indole (A-833834) and 2-(6-methyl-3,6-diazabicyclo[3.2.0]heptan-3-yl)-7-(6-methyl-3,6-diazabicyclo[3.2.0]heptan-3-yl)-9H-fluoren-9-one (A-752274) were synthesized, labeled with ^11^C (to obtain [^11^C]A-833834 and [^11^C]A-752274, respectively), and evaluated in mice (7). The biodistribution of both tracers was investigated in the mouse brain, and [^11^C]A-752274 was also evaluated for use with in vivo PET imaging of a baboon brain. This chapter presents results obtained with [^11^C]A-833834. The biodistribution and PET imaging characteristics of [^11^C]A-752274 are discussed in a separate chapter in MICAD (www.micad.nih.gov) (9).

### Related Resource Links

nAChR-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?cmd=Search&term=nAChR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log$=booksrch&bname=micad)

Human α7-nAChR (http://www.ncbi.nlm.nih.gov/gene/1139) in Gene Database; Gene ID: 1139

α7-nAChR in Online Mendelian Inheritance in Man (OMIM (http://omim.org/entry/118511)) Database

Clinical trials (http://www.clinicaltrials.gov/ct2/results?term=nAChR) related to nAChRs

nAChRs as drug targets [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?itool=pubmed_Abstract&DbFrom=pubmed&Cmd=Link&LinkName=pubmed_pubmed&IdsFromResult=21631405&retmode=ref)]

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=A-833834%20synthesis&cmd=DetailsSearch)]

The synthesis of A-833834 and its labeling with ^11^C have been described by Horti et al. (7). The total time required for the synthesis of [^11^C]A-833834 was reported to be 37 min. The identity of [^11^C]A-833834 was confirmed with coinjection of the tracer with the corresponding non-radiolabeled compound for analysis on a high-performance liquid chromatography (HPLC) column. The radiochemical yield of [^11^C]A-833834 with respect to [^11^C]methyl iodide (used to label the receptor ligand) was 32 ± 3%. The specific activity of [^11^C]A-833834 at the end of synthesis was 403 ± 70 GBq/μmol (14.9 ± 2.58 Ci/μmol), with a radiochemical purity of 96% as determined with HPLC analysis. The total synthesis time for [^11^C]A-833834 was 37 min (including the production of [^11^C]methyl iodide and quality control of the tracer).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=A-833834%20In%20Vitro%20Studies&cmd=DetailsSearch)]

The binding affinity of A-833834 for α7-nAChR was determined in a displacement assay that used rat brain membrane preparations (without the cerebellum) with [^3^H]-(S,S)-2,2-dimethyl-5-(6-phenyl-pyridazin-3-yl)-5-aza-2-azonia-bicyclo[2.2.1]heptane iodide as the radioligand (7). The K_i_ of A-833834 was reported to be 1.53 nM compared with 0.092 nM for A-752272. This indicated that the binding affinity of A-833834 was ~16-fold lower than that of A-752274 (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=A-833834%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^11^C]A-833834 was investigated in the brain tissue of normal CD1 mice (7). The animals (n = 3 animals/time point) were injected with ~100 μCi [^11^C]A-833834 through the lateral tail vein, and the rodents were euthanized at preselected time points (maximum of 60 min postinjection (p.i.)). The brains of the animals were removed, and the amount of radioactivity accumulated in the various regions of the organ was determined. Data obtained from this study were presented as percent of injected dose per gram tissue (% ID/g). The peak concentration of radioactivity in the whole brain was 1.4 ± 0.2% ID/g at 30 min p.i. Maximum accumulation of label was observed in the frontal cortex (~1.55% ID/g) at 40 min p.i., followed by the thalamus (~1.4% ID/g) and the hippocampus (1.2% ID/g) at 30 min p.i. The tissue/cerebellum uptake ratios continued to increase with time in all regions of the brain, and the frontal cortex/cerebellum uptake ratio was the highest (1.5 at 60 min p.i.). A very high accumulation of label was observed in the adrenal glands (~20% ID/g) of the animals, and this was attributed to the high expression of α7-nAChR and efficient transport in blood from these glands (compared with the different regions of the brain).

Mice (n = 3 animals/time point) were injected with a mixture of 100 μCi [^11^C]A-833834 and 3.0 mg/kg body weight non-radioactive A-83834 as described above to establish the receptor binding specificity of [^11^C]A-833834 (7). The rodents were euthanized at 60 min p.i., and the amount of radioactivity in the different regions of the brain was determined. There was an insignificant difference in the amount of radioactivity accumulated in the various regions of the brains of the control and the blocked mice. These observations indicated that [^11^C]A-833834 had a very low binding specificity for α7-nAChR in the CNS of these animals. Therefore, no further studies were performed with this tracer.

From these studies, the investigators concluded that [^11^C]A-833834 was not suitable for use as a PET probe to study the characteristics of α7-nAChR in the brain of rodents (7).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=A-833834%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=A-833834%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=A-833834%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies reported in this chapter were supported by National Institutes of Health grants DA020777 and MH079017.

## References

1 dos Santos Coura R., Granon S. (2012). Prefrontal neuromodulation by nicotinic receptors for cognitive processes. Psychopharmacology (Berl).
2 Albuquerque E.X., Pereira E.F., Alkondon M., Rogers S.W. (2009). Mammalian nicotinic acetylcholine receptors: from structure to function. Physiol Rev.
3 Kawamata J., Suzuki S., Shimohama S. (2012). alpha7 nicotinic acetylcholine receptor mediated neuroprotection in Parkinson's disease. Curr Drug Targets.
4 Hernandez C.M., Dineley K.T. (2012). alpha7 nicotinic acetylcholine receptors in Alzheimer's disease: neuroprotective, neurotrophic or both?. Curr Drug Targets.
5 Schuller H.M. (2012). Regulatory role of the alpha7nAChR in cancer. Curr Drug Targets.
6 Radek R.J., Kohlhaas K.L., Rueter L.E., Mohler E.G. (2010). Treating the cognitive deficits of schizophrenia with alpha4beta2 neuronal nicotinic receptor agonists. Curr Pharm Des.
7 Horti A.G., Ravert H.T., Gao Y., Holt D.P., Bunnelle W.H., Schrimpf M.R., Li T., Ji J., Valentine H., Scheffel U., Kuwabara H., Wong D.F., Dannals R.F. (2013). Synthesis and evaluation of new radioligands [(11)C]A-833834 and [(11)C]A-752274 for positron-emission tomography of alpha7-nicotinic acetylcholine receptors. Nucl Med Biol.
8 Horti A.G., Wong D.F. (2009). Clinical Perspective and Recent Development of PET Radioligands for Imaging Cerebral Nicotinic Acetylcholine Receptors. PET Clin.
9 Chopra, A., 2-(6-[11C]methyl-3,6-diazabicyclo[3.2.0]heptan-3-yl)-7-(6-methyl-3,6-diazabicyclo[3.2.0]heptan-3-yl)-9H-fluoren-9-one. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.